# ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-bevacizumab-IRDye 800CW

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-bevacizumab-IRDye 800CW
Abbreviated name: | ^64^Cu-NOTA-Bev-800CW
Synonym: | ^64^Cu-NOTA-p-Bn-SCN-Bev-800CW
Agent category: | Antibody
Target: | Vascular endothelial growth factor-A (VEGF-A)
Target category: | Antigen
Method of detection: | Multimodality: positron emission tomography (PET), near-infrared fluorescence (NIR) optical imaging
Source of signal: | ^64^Cu, IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF-A.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW)]

The vascular endothelial growth factor (VEGF) family is composed of five VEGF glycoproteins (VEGF-A, VEGF-B, VEGF-C, VEGF-D, and VEGF-E) and consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF-A is composed of VEGF_121_, VEGF_165_, and VEGF_189_ isoforms, which are secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like other VEGF polypeptides do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (1).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (3). Among the at least seven isoforms of VEGF-A, VEGF_121_ is freely soluble while all VEGF_189_ is bound to the cell membrane or extracellular matrix (ECM). VEGF_165_ exhibits an intermediary behavior (i.e. partly diffusible and partly bound). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease (9, 10). Therefore, it is important to measure VEGF levels in the tumors to design better anticancer treatment protocols. Bevacizumab (Bev) is a humanized antibody against VEGF-A (11) that binds to all VEGF-A isoforms, and it is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer (12). VEGFR-2 has been shown to mediate most of the VEGF-A activation in tumor endothelial cells (13, 14). Zhang et al. (15) prepared ^64^Cu-1,4,7-triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-bevacizumab-IRDye 800CW (^64^Cu-NOTA-Bev-800CW) for positron emission tomography (PET) and near-infrared fluorescence (NIR) multimodal imaging of VEGF expression in nude mice bearing U87MG human glioblastoma xenografts. U87MG cells express all three isoforms of VEGF-A (VEGF_121,_ VEGF_165,_ and VEGF_189_).

### Related Resource Links:

- Chapters in MICAD (VEGF (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VEGF+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), bevacizumab (http://www.ncbi.nlm.nih.gov/books?term=bevacizumab%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (VEGFR-2 (http://www.ncbi.nlm.nih.gov/gene/3791), VEGF (http://www.ncbi.nlm.nih.gov/gene/7422))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR-2 (http://www.ncbi.nlm.nih.gov/omim/191306), VEGF (http://www.ncbi.nlm.nih.gov/omim/192240))
- Clinical trials (bevacizumab (http://www.clinicaltrials.gov/ct2/results?term=Bevacizumab))
- Drug information in FDA (bevacizumab (http://google2.fda.gov/search?q=bevacizumab%29+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+synthesis)]

NOTA-p-Bn-SCN-Bev (NOTA-Bev) was prepared by conjugation of p-SCN-Bn-NOTA to Bev in 25:1 molar ratio at pH 9 (15). NOTA-Bev was purified with column chromatography. NOTA-Bev and IRDye 800CW-N-hydroxysuccinimide ester were incubated at 2:1 molar ratio at pH 8.5 for 2 h at room temperature. NOTA-Bev-800CW was purified with column chromatography. There were ~5 NOTA and 0.8 IRDye 800CW moieties per antibody conjugate. NOTA-Bev-800CW (0.162 nmol) was radiolabeled using 37 MBq (1 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 5.0) for 30 min at 37°C. ^64^Cu-NOTA-Bev-800CW was purified with a PD-10 column. Total preparation time of the tracer was 60 ± 10 min (n = 10). The radiochemical yield was >80%. The radiochemical purity was >98%. The specific activity of ^64^Cu-NOTA-Bev-800CW was reported to be 170 MBq/nmol (4.6 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+in+vitro)]

^64^Cu-NOTA-Bev-800CW had immunoreactivity similar to the unconjugated mAb as determined by binding to U87MG tumor cells with flow cytometry analysis (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+rodentia)]

Zhang et al. (15) studied the whole-body distribution of 5–10 MBq (0.14–27 mCi) ^64^Cu-NOTA-Bev-800CW (0.3 nmol IRDye 800CW) with PET and NIR fluorescence imaging in nude mice (n = 4/group) bearing human U87MG xenografts at 4, 24, 48, and 72 h. The U87MG tumors were clearly visualized at 24–72 h after injection. The tumor accumulation of radioactivity levels were 4.6 ± 0.7% injected dose per gram (ID/g) at 4 h, 16.3 ± 1.6% ID/g at 24 h, 18.1 ± 1.4% ID/g at 48 h, and 20.7 ± 3.7% ID/g at 72 h. The liver accumulation of radioactivity levels were 14.4 ± 3.7% ID/g at 4 h, 17.2 ± 2.0% ID/g at 24 h, 13.8 ± 2.9% ID/g at 48 h, and 12.8 ± 2.7% ID/g at 72 h. The radioactivity level in the blood was 20.5% ID/g at 4 h and decreased to 13.0% ID/g at 72 h. Pretreatment (6 h) with 13 nmol Bev inhibited accumulation of radioactivity in the U87MG tumors to <7% ID/g at 24–72 h (P < 0.01), whereas little inhibition was observed in the liver and blood. NIR fluorescence imaging was performed immediately after the PET scans, and the tumors were clearly visualized at 24–72 h. Region-of-interest analysis showed tumor NIR fluorescence radiant intensity values of 12.0 ± 3.9 × 10^6^, 19.2 ± 3.7 × 10^6^, 15.2 ± 1.9 × 10^6^, and 13.6 ± 3.9 × 10^6^ at 4, 24, 48, and 72 h, respectively. Pretreatment with Bev resulted in reduced tumor signal intensity values of 11.6 ± 1.0 × 10^6^, 8.93 ± 1.0 × 10^6^, and 7.7 ± 1.0 × 10^6^ at 24, 48, and 72 h (P < 0.05), respectively. Ex vivo PET and NIR fluorescence imaging studies were performed at 72 h. There was a linear correlation between ex vivo tumor NIR fluorescence data and in vivo PET tumor radioactivity level (% ID/g) (R^2^ = 0.93, P < 0.001). ^64^Cu-NOTA-Bev-800CW bound to VEGF that is bound to the VEGFR on the tumor cells, tumor endothelial cells and tumor ECM.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NOTA-Bev-800CW+human)]

No publication is currently available.

## NIH Support

5 T32 CA009206-32

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Gorski D.H., Beckett M.A., Jaskowiak N.T., Calvin D.P., Mauceri H.J., Salloum R.M., Seetharam S., Koons A., Hari D.M., Kufe D.W., Weichselbaum R.R. (1999). Blockage of the vascular endothelial growth factor stress response increases the antitumor effects of ionizing radiation. Cancer Res.
10 Solban N., Selbo P.K., Sinha A.K., Chang S.K., Hasan T. (2006). Mechanistic investigation and implications of photodynamic therapy induction of vascular endothelial growth factor in prostate cancer. Cancer Res.
11 Wang Y., Fei D., Vanderlaan M., Song A. (2004). Biological activity of bevacizumab, a humanized anti-VEGF antibody in vitro. Angiogenesis.
12 Ferrara N., Hillan K.J., Gerber H.P., Novotny W. (2004). Discovery and development of bevacizumab, an anti-VEGF antibody for treating cancer. Nat Rev Drug Discov.
13 Folkman J. (2002). Role of angiogenesis in tumor growth and metastasis. Semin Oncol.
14 Ferrara N., Gerber H.P., LeCouter J. (2003). The biology of VEGF and its receptors. Nat Med.
15 Zhang Y., Hong H., Engle J.W., Yang Y., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Near-Infrared Fluorescence Imaging of Vascular Endothelial Growth Factor with Dual-Labeled Bevacizumab. Am J Nucl Med Mol Imaging.